# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-cetuximab

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-cetuximab
Abbreviated name: | ^64^Cu-DOTA-cetuximab
Synonym: | ^64^Cu-DOTA-erbitux, ^64^Cu-DOTA-C225
Agent category: | Chimeric monoclonal antibody
Target: | EGF receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20Cetuximab)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab (a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody against the extracellular domain of recombinant HER2) (11) was labeled as ^111^In-trastuzumab (12-14). C225 (an anti-EGFR, mouse-human chimeric, monoclonal IgG_1_ antibody, also known as erbitux and cetuximab) was labeled as ^99m^Tc-EC-C225 (15, 16) for imaging EGFR expression on solid tumors using single-photon emission computed tomography (SPECT). However, positron emission tomography (PET) offers better sensitivity, resolution, and quantification than SPECT (17). ^64^Cu (t_1/2_ = 12.7 h, β^-^ decay) is an attractive radionuclide for labeling cetuximab. For evaluation as a PET imaging agent, ^64^Cu has been attached to cetuximab via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^64^Cu-DOTA-cetuximab.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20Cetuximab%20and%20synthesis)]

Commercially available monofunctional N-hydroxysuccinimide ester and 1-ethyl-3-[3-(dimethylamino)-propyl] carbodiimide (EDC) were used to activate DOTA to conjugate cetuximab to form DOTA-cetuximab (18), which was purified by column chromatography. DOTA per antibody was determined to be 21.5 ± 2.2. ^64^CuCl_2_ was added to DOTA-cetuximab. The reaction mixture was incubated for 60 min at 40°C. ^64^Cu-DOTA-cetuximab was purified by column chromatography. The yield of ^64^Cu-DOTA-cetuximab was 84.0 ± 8.7% with specific activities of 1.24 ± 0.13 GBq/mg (33.5 ± 3.5 mCi/mg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20Cetuximab%20and%20in%20vitro)]

Cai et al. (18) performed cell-binding assays with ^64^Cu-DOTA-cetuximab using EGFR-expressing human glioblastoma U87MG cell line. Binding of ^64^Cu-DOTA-cetuximab under antigen excess condition indicated that the immunoreactivity was 63 ± 14%, suggesting that the accessible lysine residues were largely away from the EGFR binding region of cetuximab. Ping Li et al. (19) showed that ^64^Cu-DOTA-cetuximab exhibited high binding affinity to EGFR-positive A431 cells with K_d_ of 0.28 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20Cetuximab%20and%20rodentia)]

Cai et al. studied the whole-body distribution of ^64^Cu-DOTA-cetuximab (5–10 MBq/mouse or 0.14–0.27 mCi/mouse) by microPET imaging in seven xenograft tumor models in mice with 2–20-min static scans at various time points (1–48 h) (18). ^64^Cu-DOTA-cetuximab exhibited increasing tumor activity accumulation over time in EGFR-positive tumors [>10% injected dose/g (% ID/g)] but relatively low accumulation in EGFR-negative tumors at all time points examined (<5% ID/g). The tumor uptake reached a plateau at 24 h after injection. There was a good correlation (R^2^ = 0.80) between the tracer accumulation (measured by microPET) and the EGFR expression level (measured by Western blotting). The highest activity concentrations were visualized in the liver (~15% ID/g) with little accumulation in the kidneys and muscle (<3% ID/g). The accumulation of ^64^Cu-DOTA-cetuximab was clearly visible in the tumors. No blocking experiment was performed. On the basis of the microPET imaging data obtained in Sprague-Dawley rats (n = 3), the highest radiation absorbed dose was found to be 0.41 ± 0.02 mGy/MBq (1.47 ± 0.10 rad/mCi) in the liver. Based on the rat biodistribution data, the whole-body effective dose in humans was estimated to be 0.037 ± 0.001 mGy/MBq (0.136 ± 0.003 rad/mCi).

Eiblmaier et al. (20) performed ex vivo biodistribution of ^64^Cu-DOTA-cetuximab in nude mice (n = 5) bearing CaSki cervical cancer cells at 24 h after injection. Accumulation into CaSki tumor was high (13.2 ± 1.2% ID/g). By contrast, accumulation was low in muscle (3.4% ID/g) and bone (2.6% ID/g). However, accumulation remained high in the liver (15% ID/g), blood (24% ID/g) and the spleen (26% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20Cetuximab%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20Cetuximab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Cu%20Cetuximab%20and%20human)]

No publication is currently available.

## NIH Support

P50 CA114747, R21 CA102123, R21 EB001785, R24 CA93862, U54 CA119367, R24 CA83060, P50 CA94056-04, R24 CA86307

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Lundqvist H., Tolmachev V. (2002). Targeting peptides and positron emission tomography. Biopolymers.
18 Cai, W., K. Chen, L. He, Q. Cao, A. Koong, and X. Chen, Quantitative PET of EGFR expression in xenograft-bearing mice using (64)Cu-labeled cetuximab, a chimeric anti-EGFR monoclonal antibody. Eur J Nucl Med Mol Imaging, 2007
19 Ping Li W., Meyer L.A., Capretto D.A., Sherman C.D., Anderson C.J. (2008). Receptor-binding, biodistribution, and metabolism studies of 64Cu-DOTA-cetuximab, a PET-imaging agent for epidermal growth-factor receptor-positive tumors. Cancer Biother Radiopharm.
20 Eiblmaier M., Meyer L.A., Watson M.A., Fracasso P.M., Pike L.J., Anderson C.J. (2008). Correlating EGFR expression with receptor-binding properties and internalization of 64Cu-DOTA-cetuximab in 5 cervical cancer cell lines. J Nucl Med.